# ^18^F-Labeled 6-amino-2-(4’-fluorophenyl)-1,3-benzothiazole and other derivatives

Chemical name: | ^18^F-Labeled 6-amino-2-(4’-fluorophenyl)-1,3-benzothiazole and other derivatives | [image]
Abbreviated name: | [^18^F]2 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Human amyloid β plaques | [image]
Target Category: | Protein | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-human primates | Structures of [^18^F]2, [^18^F]3 and [^18^F]6.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/pubmed?term=amyloid%20imaging%20agents&cmd=DetailsSearch)

Development of Alzheimer’s disease (AD) has been attributed to neurodegeneration as a result of the neuronal overexpression, secretion, and deposition of the neurotoxic amyloid β (Aβ) fragment of the Aβ protein precursor in the brain (1). No specific treatment for AD is currently available, and clinicians are increasingly focused on developing ways to either prevent or delay the formation of Aβ plaques in the brain of AD patients (2). In addition, several hundred clinical trials (http://clinicaltrials.gov/ct2/results?term=Alzheimer%E2%80%99s+disease+) approved by the United States Food and Drug Administration have been completed or are in progress to develop drugs for the prevention, onset delay, or treatment of AD. Early detection of Aβ plaques by non-invasive techniques such as positron emission tomography (PET) is often used to identify individuals who are prone to get the disease and also to monitor the efficacy of drugs used to treat or delay onset of the disease (3).

The ^11^C-labeled Pittsburgh compound B ([^11^C]PIB (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=PIB11C)) is the most commonly used PET tracer for detection of Aβ plaques, but due to the short half-life (20.4 min) of ^11^C the use of this label is restricted to clinical facilities that have the capability to generate the agent on-site (3). Some ^18^F-labeled compounds have also been generated for the visualization of Aβ plaques, but these labeled compounds have low specificity (3), and the PIB analogs [^18^F]BAY94-9172 (4) and [^18^F]GE067 (5) or its derivative, [^18^F]flutemetamol (6), are currently under clinical evaluation. In an ongoing effort to develop ^18^F-labeled compounds for the detection of Aβ plaques and to monitor the efficacy of drugs used to treat AD, Serdons et al. (3) synthesized three new ^18^F-labeled derivatives of 2-phenylbenzothiazoles (designated [^18^F]2, [^18^F]3, and [^18^F]6, respectively), determined the in vitro affinity of these tracers for Aβ fibrils, and investigated their biodistribution in mice, pharmacokinetics in rats, and pharmacokinetics and uptake in monkeys.

### Other sources of information regarding human β amyloid protein

β Amyloid plaques in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Beta%20amyloid%20plaques).

Human β amyloid protein (http://www.ncbi.nlm.nih.gov/protein/P05067.3?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=351&log$=databasead1&logdbfrom=nuccore) sequence.

Alzheimer’s disease in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Alzheimer%E2%80%99s%20disease%20).

Alzheimer’s disease in Genome Wide Association Studies (http://www.genome.gov/gwastudies/index.cfm?#searchForm) database.

FDA-approved treatments (http://www.alz.org/national/documents/topicsheet_treatments.pdf) for Alzheimer’s disease (from Alzheimer’s Association web site; www.alz.org).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20derivatives%20of%202-phenylbenzothiazoles&cmd=DetailsSearch)]

The synthesis processes of [^18^F]2 (6-amino-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole), [^18^F]3 , (6-methylamino-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole) and [^18^F]6 (6-dimethylamino-2-(4’-[^18^F]fluorophenyl)-1,3-benzothiazole), respectively, were described by Serdons et al. (3). The identity of the labeled compounds was confirmed by co-elution with the appropriate unlabeled compound using the same analytical high-performance liquid chromatography (HPLC) procedure. The time taken to obtain the pure products was reported to be between 75 and 100 min. The radiochemical purity of the tracers was reported to be >99% with a yield of 10.5 ± 5.2% for [^18^F]2 (specific activity, 72 GBq/μmol (1.945 Ci/μmol)), 45.0 ± 12.5% for [^18^F]3 (specific activity, 82 GBq/μmol (2.216 Ci/μmol)), and 19.3 ± 9.0% for [^18^F]6 (specific activity, 24 GBq/μmol (0.648 Ci/μmol)).

In some studies, [^11^C]PIB and [^18^F]KS28 were also used for comparison with [^18^F]2, [^18^F]3, and [^18^F]6 (3). However, the synthesis, radiochemical purity, yield, specific activity, and stability of [^11^C]PIB and [^18^F]KS28 were not reported.

The in vivo stability of [^18^F]2, [^18^F]3, and [^18^F]6 was studied in normal mice and monkeys and has been described in the appropriate Animal Studies subsections of below.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-%28methyl%29amino-2-%284%u2019-fluorophenyl%29-1%2C3-benzothiazole%20in%20vitro%20studies&cmd=DetailsSearch)]

Using human AD brain homogenates in a [^125^I]IMPY competition assay, the in vitro affinities of unlabeled compounds 2, 3, and 6 for Aβ fibrils were determined by Serdons et al. (3). The inhibition constant values for compounds 2, 3, and 6 were reported to be 10.0 ± 1.0, 4.1 ± 0.3, and 3.8 ± 0.4 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

To investigate the brain pharmacokinetics of the labeled Aβ-targeting compounds, the biodistribution of [^18^F]2, [^18^F]3, and [^18^F]6 was compared to that of [^11^C]PIB and [^18^F]KS28 at 2 min and 60 min after intravenous (i.v.) injection of the respective tracers in normal mice (n = 4–6 animals/tracer per time point) as described by Serdons et al. (3). Data are presented as a percentage of injected dose per gram tissue (% ID/g); for complete biodistribution of the radiolabeled compounds in mice, see Tables 2, 3, 4, 5, and 6 in Serdons et al. (3). Among the Aβ tracers, [^18^F]2 had the highest uptake in the cerebrum (13.97 ± 0.63% ID/g) at 2 min postinjection (p.i.), followed by [^18^F]3 (12.13 ± 0.48% ID/g) and [^18^F]6 (8.84 ± 0.91% ID/g). The brain uptake of the three labeled Aβ binding compounds was significantly higher (P < 0.05, two-sided) than either [^11^C]PIB (3.60 ± 1.40% ID/g) or [^18^F]KS28 (5.33 ± 0.74% ID/g). Also, the brain uptake of [^18^F]2 > [^18^F]3 > [^18^F]6 (P < 0.05, two-sided, between each compound). The ratios of accumulated radioactivity in the cerebrum at 2 min and 60 min for [^18^F]2, [^18^F]3, and [^18^F]6 were 14.2, 7.8, and 4.5 respectively. Also, for [^18^F]2 this ratio was four-fold and three-fold higher than for [^11^C]PIB and [^18^F]KS28, respectively. This indicated that the washout of radioactivity from the brain for [^18^F]2 was slower than that of all the other tracers. In another study, animals pretreated with unlabeled compound 2 followed by an injection of [^18^F]2 (the time difference between the pretreatment and injection of the radiolabeled compound was not reported) showed there was no significant difference (P < 0.05, two-sided) in the biodistribution of radioactivity between the pretreated and the untreated animals at 60 min p.i., suggesting that the radioactivity accumulated at 60 min p.i. was probably due to nonspecific binding of the label. The clearance of [^18^F]2 from the blood was reported to be faster than that of either [^11^C]PIB or [^18^F]KS28. In addition, the radioactivity from the different compounds was cleared from the plasma primarily through the hepatobiliary system, and a small fraction was excreted through the urine.

The in vivo stability of the various Aβ tracers was investigated with HPLC analysis of the plasma and brain of normal mice. Samples were obtained from the animals at 2, 10, 30, and 60 min (n = 3 animals/time point) after an i.v. injection of the respective tracers (3). The percentages of intact [^18^F]KS28, [^18^F]2, [^18^F]3, and [^18^F]6 in the plasma were 3.2 ± 1.7, 16.5 ± 2.0, 4.1 ± 1.4, and 6.0 ± 6.4, respectively, at 60 min p.i. The ^18^F-labeled compounds 2, 3, and 6 were reported to have at least two, three, and four metabolites, respectively, in the plasma as determined with reverse-phase (RP)-HPLC. The percentages of intact [^18^F]KS28, [^18^F]2, [^18^F]3, and [^18^F]6 in the brain were 86.2 ± 2.5, 86.3 ± 0.0, 60.3 ± 3.9, and 59.2 ± 17.9, respectively, at 60 min p.i. as determined with RP-HPLC. This observation indicated that the radiometabolites of [^18^F]2 did not efficiently cross the blood–brain barrier (BBB) in the mice.

To investigate the brain pharmacokinetics of the new ^18^F-labeled Aβ binding tracers, micro-PET (μPET) imaging was performed on a normal male Wistar rat (under anesthesia with isoflurane in oxygen) injected with either [^18^F]2, [^18^F]3, or [^18^F]6 through the tail vein (time interval of 1 d or 3 d between each radiocompound injection) as described by Serdons et al. (3). Dynamic μPET images of the animal were acquired at 120 min p.i. Data obtained from this study were compared to data obtained earlier with [^11^C]PIB and [^18^F]KS28, respectively, during a μPET imaging study (7). For a blocking study, a spontaneously breathing rat was given an intraperitoneal injection of excess (0.35 mg) unlabeled compound 2 followed by i.v. injection of [^18^F]2 30 min later, and μPET images were obtained as before. Time-activity curves for the various tracers in the frontotemporal cortex of the animal were obtained, and the values were expressed as standard uptake values (SUVs). The brain uptake values of [^18^F]2, [^18^F]3, or [^18^F]6 were reported to be approximately two-fold higher than either [^11^C]PIB or [^18^F]KS28 at 2 min p.i. A comparison of the SUVs for the mouse cerebrum (for details see above) and the rat frontotemporal cortex were similar, but at 60 min p.i. these values were lower for the mice than those obtained with the rats, indicating there was an interspecies difference in clearance of the labeled compounds from the brain of these animals. Similar to the biodistribution study with mice, no significant (P < 0.05, two-sided) difference between the SUVs of the pretreated and the untreated rats was noticed, indicating that the prolonged retention of [^18^F]2 was due to nonspecific binding of radioactivity. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-phenylbenzothiazoles%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-phenylbenzothiazoles%20Non-Human%20Primates&cmd=DetailsSearch)]

Because of the interspecies brain washout differences observed with the mice and rats, the brain uptake values of [^18^F]2, [^18^F]3, and [^18^F]6 were studied with μPET imaging in a normal rhesus monkey (Maccaca mulatta; initially sedated with ketamine and later anesthetized with isoflurane) (3). The monkey was injected with [^18^F]2, [^18^F]3, [^18^F]6, or [^11^C]PIB through the vena saphena with a 1-d interval between each tracer. Dynamic μPET imaging was performed for 180 min with [^18^F]2, [^18^F]3, and [^18^F]6 and for 90 min for [^11^C]PIB. Data analysis was performed as described for the rat μPET study (see above). None of the new tracers were detected in the monkey skull, indicating that these labeled compounds or their metabolites did not cross the BBB. For a detailed description and discussion of the results from this study, see Serdons et al. (3). Briefly, although [^18^F]3 had the highest initial uptake, [^18^F]2 had the fastest clearance from the brain. In addition, [^18^F]2 had the highest ratio between the cerebrum and the brain white matter, indicating that this radiolabeled compound had the lowest nonspecific binding in the monkey white matter, which is considered a favorable characteristic for the detection of Aβ plaques by imaging in AD patients.

The pharmacokinetics of [^18^F]2, [^18^F]3, [^18^F]6, and [^11^C]PIB were investigated in monkey plasma by analyzing samples taken at different time points (varying from 2–180 min p.i.) as described by Serdons et al. (3). Among the new Aβ tracers, only [^18^F]2 was 66.9% intact at 180 min after the injection as determined with RP-HPLC(at 2 min [^18^F]2 was 91.8% intact), and its rate of metabolism was comparable to that of [^11^C]PIB (3).

On the basis of the results obtained from this study, Serdons et al. concluded that [^18^F]2 is probably a suitable PET imaging agent for the detection of Aβ plaques in AD patients (3). However, it is appropriate to mention here that the use of this labeled compound in humans will have to be evaluated in clinical trials before [^18^F]2 can be utilized for the detection of Aβ plaques in humans.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-phenylbenzothiazoles%20Human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Bissette G. (2009). Does Alzheimer's disease result from attempts at repair or protection after transient stress?. J Alzheimers Dis.
2 Sano M., Grossman H., Van Dyk K. (2008). Preventing Alzheimer's disease : separating fact from fiction. CNS Drugs.
3 Serdons K., Van Laere K., Janssen P., Kung H.F., Bormans G., Verbruggen A. (2009). Synthesis and evaluation of three 18F-labeled aminophenylbenzothiazoles as amyloid imaging agents. J Med Chem.
4 Rowe C.C., Ackerman U., Browne W., Mulligan R., Pike K.L., O'Keefe G., Tochon-Danguy H., Chan G., Berlangieri S.U., Jones G., Dickinson-Rowe K.L., Kung H.P., Zhang W., Kung M.P., Skovronsky D., Dyrks T., Holl G., Krause S., Friebe M., Lehman L., Lindemann S., Dinkelborg L.M., Masters C.L., Villemagne V.L. (2008). Imaging of amyloid beta in Alzheimer's disease with 18F-BAY94-9172, a novel PET tracer: proof of mechanism. Lancet Neurol.
5 Koole M., Lewis D.M., Buckley C., Nelissen N., Vandenbulcke M., Brooks D.J., Vandenberghe R., Van Laere K. (2009). Whole-body biodistribution and radiation dosimetry of 18F-GE067: a radioligand for in vivo brain amyloid imaging. J Nucl Med.
6 Nelissen N., Van Laere K., Thurfjell L., Owenius R., Vandenbulcke M., Koole M., Bormans G., Brooks D.J., Vandenberghe R. (2009). Phase 1 study of the Pittsburgh compound B derivative 18F-flutemetamol in healthy volunteers and patients with probable Alzheimer disease. J Nucl Med.
7 Serdons K., Terwinghe C., Vermaelen P., Van Laere K., Kung H., Mortelmans L., Bormans G., Verbruggen A. (2009). (18)F-Labeled 2-Phenylbenzothiazoles as Positron Emission Tomography Imaging Agents for Amyloid Plaques in Alzheimer's Disease. J Med Chem.